# ^188^Re-Labeled humanized monoclonal anti-epidermal growth factor receptor antibody

Chemical name: | ^188^Re-Labeled humanized monoclonal anti-epidermal growth factor receptor antibody
Abbreviated name: | ^188^Re-Nimotuzumab
Synonym: | ^188^Re-labeled monoclonal antibody nimotuzumab
Agent Category: | Monoclonal antibody
Target: | Epidermal growth factor receptor (EGFR)
Target Category: | Receptor-antibody binding
Method of detection: | Single-photon emission computed tomography (SPECT); planar gamma imaging
Source of Signal/Contrast: | ^188^Re
Activation: | No
Studies: | - In vitro; - Humans | Click for protein and nucleotide information (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=1956&log$=databasead&logdbfrom=protein) on the human EGFR.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=188re+nimotuzumabhttp://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D)]

Overexpression of the epidermal growth factor receptor (EGFR) is a characteristic feature of a variety of cancers such as lung, breast, ovarian, head and neck, bladder, and colon cancers (1). EGFR is a 170-kDa transmembrane protein that promotes cell proliferation through a receptor-associated tyrosine kinase–mediated signal transduction pathway that is activated by the specific binding of autocrine molecules such as epidermal growth factor (EGF) and transforming growth factor α (TGFα). An increased activity of these factors is believed to contribute to the progression of cancers. There are indications that EGFR polymorphism is associated with differences in the in vitro toxicity of various DNA-interfering drugs that are used for the treatment of cancer (2). In an effort to develop therapy against cancer, a variety of EGFR inhibitors have been created that either inhibit activation of the receptor kinase or inhibit the binding of EGF and TGFα (e.g., monoclonal antibodies (MAb) to the receptor) (3). In addition, efforts are under way to develop EGFR-based vaccines for the treatment of cancer patients with EGFR-positive tumors (4). EGFR is the target for treating various cancers in a variety of clinical trials (http://clinicaltrials.gov/ct2/results?term=EGFR) approved by the United States Food and Drug Administration.

The murine MAb ior egf/r3, which has a high affinity for an extracellular domain of EGFR, was developed and tested for the treatment of cancers (5). This MAb was also labeled with radioactive technetium (^99m^Tc) for molecular imaging of EGFR in tumors to possibly predict responses to a variety of therapeutic agents under development for the treatment of cancers (6). However, because of its immunogenicity, the ^99m^Tc-labeled ior egf/r3 MAb has limited clinical utility, particularly if repeated imaging investigations are necessary (5). To circumvent this problem, a humanized form of ior egf/r3 was developed by combining the complimentary determining regions of the murine antibody with a human immunoglobulin-1 framework (7). This humanized antibody, designated as nimotuzumab, has a low affinity for the receptor; with modification of the hR3 structure, an antibody with a similar receptor affinity as the original murine MAb was obtained. The hR3 was subsequently labeled with ^99m^Tc and investigated for its tissue distribution and imaging properties (5, 8).

Nimotuzumab was also labeled with rhenium (^188^Re) because this radionuclide can serve as a dual-purpose agent that can be used for the treatment of cancers and for scintigraphic tumor imaging (it is a 15% γ-emitter with a high-energy β emission) (9). The biodistribution of ^188^Re-labeled nimotuzumab was investigated using single-photon emission computed tomography after locoregional administration in patients with high-grade gliomas (tumors in the brain).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=188Re+nimotuzumab+synthesis)]

The humanized MAb nimotuzumab was developed and produced as described by Mateo et al. (7). The MAb was reduced with mercaptoethanol (2-ME) as described by Morales et al. (10). Nimotuzumab was mixed with 2,000-fold excess of 2-ME and incubated for 30 min at room temperature. The reduced MAb was then purified on a PD-10 gel filtration column and eluted in nitrogen-purged phosphate-buffered saline (pH 8.2). A solution containing sodium glucoheptonate, ascorbic acid, and stannous fluoride was then added to the purified and reduced MAb. To label the agent, ^188^Re was added to the mixture and incubated for 3 h at room temperature. The amount of labeled glucoheptonate and perrhenate was determined with paper chromatography after the labeling reaction as described (10). The radiochemical yield, radiochemical purity, the specific activity, and stability of ^188^Re-nimotuzumab were not reported (9).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=188Re+nimotuzumab+in+vitro)]

No references are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=188Re+nimotuzumab+rodentia)]

No references are currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=188Re+nimotuzumab+non+primate+mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=188Re+nimotuzumab+non+human+primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=188Re+nimotuzumab+humans)]

The biodistribution of ^188^Re-nimotuzumab was investigated with locoregional radioimmunotherapy in a phase I, open-labeled, uncontrolled, dose-escalation study in nine patients with grade III or grade IV gliomas (9). The labeled MAb was administered as a bolus to the patients through a subcutaneous reservoir implanted after craniotomy. As a prophylactic, all patients received a treatment of dexamethasone and diuretics (to promote clearance of the labeled drug) starting 72 h before administration of the labeled MAb. Planar images of the anterior and posterior views of the whole body were acquired 1, 5, 24, and 48 h after administration of the labeled MAb. The uptake of radioactivity was reported as a percent of injected doses (% ID) in the tumor region and the main source organs. From the images it was calculated that 85.5 ± 10.3% ID of ^188^Re-nimotuzumab was retained in the tumor cavity and adjacent tissues 1 h after administration. The biological half-life of the activity in the tumor cavity was ~22.7 ± 8.9 h. The liver and kidneys had an uptake of 5.6% ID and 4.6% ID, respectively, 48 h after the label was administered to the patients. During the first 48 h after administration of the labeled MAb, ~6.2 ± 0.8% ID was excreted through the urine. At 48 h, ~0.5% ID of the label was found in blood circulation of the treated patients.

## Supplemental Information

[Disclaimers]

## References

1 Gullick W.J. (1991). Prevalence of aberrant expression of the epidermal growth factor receptor in human cancers. Br Med Bull.
2 Puyo S., Le Morvan V., Robert J. (2008). Impact of EGFR Gene Polymorphisms on Anticancer Drug Cytotoxicity In Vitro. Mol Diagn Ther.
3 Dancey J.E. (2003). Recent advances of molecular targeted agents: opportunities for imaging. Cancer Biol Ther.
4 Ramirez B.S., Alpizar Y.A., Fernandez D.R., Hidalgo G.G., Capote A.R., Rodriguez R.P., Fernandez L.E. (2008). Anti-EGFR activation, anti-proliferative and pro-apoptotic effects of polyclonal antibodies induced by EGFR-based cancer vaccine. Vaccine.
5 Vallis K.A., Reilly R.M., Chen P., Oza A., Hendler A., Cameron R., Hershkop M., Iznaga-Escobar N., Ramos-Suzarte M., Keane P. (2002). A phase I study of 99mTc-hR3 (DiaCIM), a humanized immunoconjugate directed towards the epidermal growth factor receptor. Nucl Med Commun.
6 Ramos-Suzarte M., Rodriguez N., Oliva J.P., Iznaga-Escobar N., Perera A., Morales A., Gonzalez N., Cordero M., Torres L., Pimentel G., Borron M., Gonzalez J., Torres O., Rodriguez T., Perez R. (1999). 99mTc-labeled antihuman epidermal growth factor receptor antibody in patients with tumors of epithelial origin: Part III. Clinical trials safety and diagnostic efficacy. J Nucl Med.
7 Mateo C., Moreno E., Amour K., Lombardero J., Harris W., Perez R. (1997). Humanization of a mouse monoclonal antibody that blocks the epidermal growth factor receptor: recovery of antagonistic activity. Immunotechnology.
8 Torres L.A., Perera A., Batista J.F., Hernandez A., Crombet T., Ramos M., Neninger E., Perez M., Sanchez E.L., Romero S., Aguilar V., Coca M.A., Iznaga-Escobar N. (2005). Phase I/II clinical trial of the humanized anti-EGF-r monoclonal antibody h-R3 labelled with 99mTc in patients with tumour of epithelial origin. Nucl Med Commun.
9 Torres L.A., Coca M.A., Batista J.F., Casaco A., Lopez G., Garcia I., Perera A., Pena Y., Hernandez A., Sanchez Y., Romero S., Leyva R., Prats A., Fernandez R. (2008). Biodistribution and internal dosimetry of the 188Re-labelled humanized monoclonal antibody anti-epidemal growth factor receptor, nimotuzumab, in the locoregional treatment of malignant gliomas. Nucl Med Commun.
10 Morales A.A., Crespo F.Z., Gandolff G.N., Iznaga Escobar N., Perez N.P., Hernandez J.C. (1998). Technetium-99m direct radiolabeling of monoclonal antibody ior egf/r3. Nucl Med Biol.